# Biotinylated vascular endothelial growth factor_121_-Avi-streptavidin-IRDye800

Chemical name: | Biotinylated vascular endothelial growth factor_121_-Avi-streptavidin-IRDye800
Abbreviated name: | VEGF_121_-Avib-SA800
Synonym:
Agent category: | Polypeptide
Target: | VEGF receptor
Target category: | Receptor
Method of detection: | Optical, near-infrared (NIR) fluorescence imaging
Source of signal: | IRDye800
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=71051581), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_001025368.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=7422) for more information about VEGF.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VEGF-Avib)]

Optical fluorescence imaging is increasingly being used to monitor biological functions of specific targets in small animals (1-3). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the natural background fluorescence interference of biomolecules, providing a high contrast between target and background tissues in small animals. NIR fluorophores have a wider dynamic range and minimal background fluorescence as a result of reduced scattering compared with visible fluorescence detection. NIR fluorophores also have high sensitivity, attributable to low background fluorescence, and high extinction coefficients, which provide high quantum yields. The NIR region is compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is a non-invasive complement to radionuclide imaging in small animals.

Vascular endothelial growth factor (VEGF) consists of at least six isoforms of various numbers of amino acids (121, 145, 165, 183, 189, and 206 amino acids) produced through alternative splicing (4). VEGF_121_, VEGF_165_, and VEGF_189_ are the forms secreted by most cell types and are active as homodimers linked by disulfide bonds. VEGF_121_ does not bind to heparin like the other VEGF species (5). VEGF is a potent angiogenic factor that induces proliferation, sprouting, migration, and tube formation of endothelial cells. There are three high-affinity tyrosine kinase VEGF receptors (VEGFR-1, Flt-1; VEGFR-2, KDR/Flt-1; and VEGFR-3, Flt-4) on endothelial cells. Several types of non-endothelial cells such as hematopoietic stem cells, melanoma cells, monocytes, osteoblasts, and pancreatic β cells also express VEGF receptors (4).

VEGF receptors were found to be overexpressed in various tumor cells and tumor-associated endothelial cells (6). Inhibition of VEGF receptor function has been shown to inhibit pathological angiogenesis as well as tumor growth and metastasis (7, 8). Radiolabeled VEGF tracers have been developed for imaging solid tumors and angiogenesis in humans (9-11). Wang et al. (12) fused the Avi peptide (14 amino acids) to the C-terminus of VEGF_121_ to allow site-specific biotinylation of the epsilon amine group of a central lysine residue of Avi. The binotinylated VEGF_121_-Avi (VEGF_121_-Avib) was able to form a tight complex with streptavidin-IRDye800 (SA800) as VEGF_121_-Avib-SA800 for NIR imaging of VEGFR expression in vivo to study tumor angiogenesis.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VEGF-Avib+synthesis)]

Wang et al. (12) constructed the fusion gene encoding VEGF_121_-Avi with DNA recombinant technology. The purified fusion protein was incubated with BirA enzyme for biotinylation for 30 min at 30ºC to form VEGF_121_-Avib. There was one biotin molecule per VEGF_121_-Avib protein. SA-IRDye800 contains 2.4 dye molecules per SA molecule.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VEGF-Avib+in+vitro)]

In vitro competition binding studies were performed with porcine aortic endothelial cells expressing cloned human VEGFR-2 using ^125^I-VEGF_165_ as the radioactive ligand (12). The binding affinity values of VEGF_121_, VEGF_121_-Avi, VEGF_121_-Avib-SA800, and VEGF_121_-Avi-IRDye800 (IRDye800 chemically conjugated) were 0.72 ± 0.41, 5.18 ± 1.29, 3.09 ± 1.15, and 3,030 ± 790 nM, respectively. The binding affinity of VEGF_121_-Avib-SA800 was only slightly lower than that of VEGF_121_, whereas the binding affinity of VEGF_121_-Avi-IRDye800 was >1,000-fold lower than that of VEGF_121_.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VEGF-Avib+rodentia)]

Wang et al. (12) performed in vivo NIR fluorescence imaging studies of VEGF_121_-Avib-SA800, VEGF_m_-Avib-SA800 (non-active VEGF mutant), VEGF_121_-Avi-IRDye800 (less active than VEGF121 as binding affinity was decreased with the direct conjugation of IRDye800), and SA800 (0.5 nmol IRDye800 equivalent per mouse) in mice (n = 4/group) bearing VEGFR-2–expressing 67NR murine breast tumors. Sagittal images were obtained at 2, 18, 40, and 66 h after intravenous injection. VEGF_121_-Avib-SA800 exhibited peak signal intensity at 18 h with a gradual washout. The tumor/muscle ratios for VEGF_121_-Avib-SA800 were 6–7 at these time points, whereas VEGF_m_-Avib-SA800, VEGF_121_-Avi-IRDye800, and SA800 exhibited tumor/muscle ratios of <2 at these time points. No blocking experiment was performed. Ex vivo NIR fluorescence images of various organs were obtained at 66 h after injection. The normalized light intensity signal was 3.5 in the tumor with VEGF_121_-Avib-SA800. The organs with the highest NIR signal were the kidneys (7.5) and liver (4.9), with little signal in the lung (0.6), spleen (1.0), and heart (1.1). The tumor/muscle ratios were 4, 1, 1, and 1 for VEGF_121_-Avib-SA800, VEGF_m_-Avib-SA800, VEGF_121_-Avi-IRDye800, and SA800, respectively. Immunofluorescence staining confirmed the colocalization of VEGF-Avib-SA-Cy5.5 with the luminal endothelial cells in the tumor.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VEGF-Avib+and+(dog+or+sheep+or+pig+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VEGF-Avib+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VEGF-Avib+human)]

No publication is currently available.

## NIH Support

P50 CA114747, U54 CA119367

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
3 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
4 Ferrara N. (2004). Vascular endothelial growth factor: basic science and clinical progress. Endocr Rev.
5 Cohen T., Gitay-Goren H., Sharon R., Shibuya M., Halaban R., Levi B.Z., Neufeld G. (1995). VEGF121, a vascular endothelial growth factor (VEGF) isoform lacking heparin binding ability, requires cell-surface heparan sulfates for efficient binding to the VEGF receptors of human melanoma cells. J Biol Chem.
6 Soria J.C., Fayette J., Armand J.P. (2004). Molecular targeting: targeting angiogenesis in solid tumors. Ann Oncol.
7 Ferrara N. (2004). Vascular endothelial growth factor as a target for anticancer therapy. Oncologist.
8 Hicklin D.J., Ellis L.M. (2005). Role of the vascular endothelial growth factor pathway in tumor growth and angiogenesis. J Clin Oncol.
9 Li S., Peck-Radosavljevic M., Koller E., Koller F., Kaserer K., Kreil A., Kapiotis S., Hamwi A., Weich H.A., Valent P., Angelberger P., Dudczak R., Virgolini I. (2001). Characterization of (123)I-vascular endothelial growth factor-binding sites expressed on human tumour cells: possible implication for tumour scintigraphy. Int J Cancer.
10 Li S., Peck-Radosavljevic M., Kienast O., Preitfellner J., Hamilton G., Kurtaran A., Pirich C., Angelberger P., Dudczak R. (2003). Imaging gastrointestinal tumours using vascular endothelial growth factor-165 (VEGF165) receptor scintigraphy. Ann Oncol.
11 Li S., Peck-Radosavljevic M., Kienast O., Preitfellner J., Havlik E., Schima W., Traub-Weidinger T., Graf S., Beheshti M., Schmid M., Angelberger P., Dudczak R. (2004). Iodine-123-vascular endothelial growth factor-165 (123I-VEGF165). Biodistribution, safety and radiation dosimetry in patients with pancreatic carcinoma. Q J Nucl Med Mol Imaging.
12 Wang H., Chen K., Niu G., Chen X. (2009). Site-specifically biotinylated VEGF(121) for near-infrared fluorescence imaging of tumor angiogenesis. Mol Pharm.